# 1-(2,4-Dichlorophenyl)-4-cyano-5-(4-[^11^C]methoxyphenyl)-N-(pyrrolidin-1-yl)-1H-pyrazole-3-carboxamide

Chemical name: | 1-(2,4-Dichlorophenyl)-4-cyano-5-(4-[^11^C]methoxyphenyl)-N-(pyrrolidin-1-yl)-1H-pyrazole-3-carboxamide
Abbreviated name: | [^11^C]JHU76609
Synonym:
Agent category: | Compound
Target: | Cannabinoid CB1 receptors
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528)]

There are two subtypes of cannabinoid receptors in mammalian tissues: CB1 and CB2 (1, 2). CB1 receptors are expressed abundantly in neuronal terminals in the central nervous system (CNS) and in some peripheral tissues to inhibit neurotransmitter release. CB1 receptors are found predominately in the striatum, hippocampus, substantia nigra, globus pallidus, and cerebellum. CB2 receptors are present mainly on immune cells to modulate cytokine release. Both receptor subtypes are coupled through G_i/o_ proteins to inhibit adenylate cyclase and to modulate potassium and calcium channels. CB1 receptors have been demonstrated to be involved in analgesia, regulation of food intake, and control of movement in normal subjects (3). Alternation of CB1 receptor function has been implicated in a number of human diseases such as depression, schizophrenia, and obesity (4-6).

Δ9-Tetrahydrocannabinol (THC) is a major active cannabinoid found in marijuana and activates CB1 receptors (7). THC has a very high lipophilicity (log D_7.4_ value of 7), which causes imaging studies using radiolabeled THC to be unsuccessful because of slow entry into the brain and high nonspecific binding. However, a high lipophilicity is essential for binding to CB1 receptors, and an optimal lipophilicity (log D_7.4_ 1–4) is required for crossing the blood–brain barrier (BBB). Existing radiolabeled ligands are mainly analogs of the antagonist rimonabant (SR141716A) and the agonist WIN 55,212-2, which also exhibit high nonspecific binding and lipophilicity, limiting their application in imaging (8). Therefore, there is a need to lower the lipophilicity of the CB1 radioligands with little effect on binding affinity and ability to cross the BBB. 4-Cyano-1-(2,4-dichlorophenyl)-5-(4-methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide (JHU75528), an analog of SR141716A, is a potent and selective CB1 antagonist with nanomolar affinity and lower lipophilicity than SR141716A (9). 4-Cyano-1-(2,4-dichlorophenyl)-5-(4-[^11^C]methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide ([^11^C]JHU75528) has been studied as a positron emission tomography agent for the non-invasive study of CB1 receptors in the brain with moderate binding (10). 1-(2,4-Dichlorophenyl)-4-cyano-5-(4-[^11^C]methoxyphenyl)-N-(pyrrolidin-1-yl)-1H-pyrazole-3-carboxamide ([^11^C]JHU76609), an analog of [^11^C]JHU75528, is being evaluated for use as a CB1 tracer (11).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=CB1+AND+micad%5Bbook%5D)
- Gene information in NCBI (CB1 receptors (http://www.ncbi.nlm.nih.gov/gene/1268))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/114610)
- Clinical trials (CB1 (http://www.clinicaltrials.gov/ct2/results?term=CB1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20synthesis)]

Fan et al. (11) reported the synthesis of [^11^C]JHU76609 by reaction of the nor-methyl precursor 1-(2,4-dichlorophenyl)-4-cyano-5-(4-hydroxyphenyl)-N-(pyrrolidin-1-yl)-1H-pyrazole-3-carboxamide with [^11^C]methyl triflate for 3 min at 45°C in acetone in the presence of 2 M sodium hydroxide. An average radiochemical yield was 15–24% (non–decay-corrected) with a total synthesis time of ~30 min after purification by column chromatography. Specific activities were 482 ± 288 GBq/μmol (13.0 ± 7.8 Ci/μmol) at the end of synthesis with a radiochemical purity of >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20in%20vitro)]

Fan et al. (10) reported that JHU75528 had a K_i_ value of 11 ± 7 nM and a log D_7.4_ (lipophilicity) value of 3.6 ± 0.3. As a reference, K_i_ and log D_7.4_ values were 35–46 nM and 4.6 ± 0.8 for SR141716A, respectively. JHU76609 exhibited K_i_ and log D_7.4_ values of 2.0–3.7 nM and 2.8 ± 0.1, respectively (11). Therefore, JHU76609 displayed higher binding affinity and lower lipophilicity than JHU75528.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20rodentia)]

Fan et al. (11) performed ex vivo biodistribution studies in male CD-1 mice (n = 3) at 30, 45, and 90 min after injection of 7.4 MBq (0.2 mCi) [^11^C]JHU76609. The hippocampus, cortex, and cerebellum exhibited high accumulation (~5% injected dose/g (ID/g) at 30 min). The brain stem had the lowest accumulation (~2% ID/g at 30 min). Peak concentration of radioactivity occurred at 15–20 min followed by washout. The hippocampus/brain stem ratios were 2.3, 3.0, and 3.5 at 30, 60, and 90 min after injection, respectively. Pretreatment with 1 mg/kg SR141716A 15 min before tracer injection reduced the hippocampus uptake nearly to background level at 60 min after injection. On the other hand, no inhibition was observed in the brain stem.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20human)]

No publication is currently available.

## NIH Support

DA-021358, DA-03934, MH-079017

## References

1 Howlett A.C., Barth F., Bonner T.I., Cabral G., Casellas P., Devane W.A., Felder C.C., Herkenham M., Mackie K., Martin B.R., Mechoulam R., Pertwee R.G. (2002). International Union of Pharmacology. XXVII. Classification of cannabinoid receptors. Pharmacol Rev.
2 Pertwee R.G. (1997). Pharmacology of cannabinoid CB1 and CB2 receptors. Pharmacol Ther.
3 Pertwee, R.G., Pharmacological actions of cannabinoids. Handb Exp Pharmacol, 2005(168): p. 1-51.
4 Gambi F., De Berardis D., Sepede G., Quartesan R., Calcagni E., Salerno R.M., Conti C.M., Ferro F.M. (2005). Cannabinoid receptors and their relationships with neuropsychiatric disorders. Int J Immunopathol Pharmacol.
5 De Vries T.J., Schoffelmeer A.N. (2005). Cannabinoid CB1 receptors control conditioned drug seeking. Trends Pharmacol Sci.
6 Guzman M., Sanchez C. (1999). Effects of cannabinoids on energy metabolism. Life Sci.
7 Martin B.R. (1986). Cellular effects of cannabinoids. Pharmacol Rev.
8 Gifford A.N., Makriyannis A., Volkow N.D., Gatley S.J. (2002). In vivo imaging of the brain cannabinoid receptor. Chem Phys Lipids.
9 Horti A.G., Fan H., Kuwabara H., Hilton J., Ravert H.T., Holt D.P., Alexander M., Kumar A., Rahmim A., Scheffel U., Wong D.F., Dannals R.F. (2006). 11C-JHU75528: a radiotracer for PET imaging of CB1 cannabinoid receptors. J Nucl Med.
10 Fan H., Ravert H.T., Holt D.P., Dannals R.F., Horti A.G. (2006). Synthesis of 1-(2,4-dichlorophenyl)-4-cyano-5-(4-[11C]methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide ([11C]JHU75528) and 1-(2-bromophenyl)-4-cyano-5-(4-[11C]methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide ([11C]JHU75575) as potential radioligands for PET imaging of cerebral cannabinoid receptor. Journal of Labelled Compounds and Radiopharmaceuticals.
11 Fan H., Kotsikorou E., Hoffman A.F., Ravert H.T., Holt D., Hurst D.P., Lupica C.R., Reggio P.H., Dannals R.F., Horti A.G. (2009). Analogs of JHU75528, a PET ligand for imaging of cerebral cannabinoid receptors (CB1): development of ligands with optimized lipophilicity and binding affinity. Eur J Med Chem.